# Ultrasmall superparamagnetic iron oxide-cyclo(Cys-Asn-Asn-Ser-Lys-Ser-His-Thr-Cys)

Chemical name: | Ultrasmall superparamagnetic iron oxide-cylco(Cys-Asn-Asn-Ser-Lys-Ser-His-Thr-Cys)
Abbreviated name: | USPIO-R832
Synonym: | P03011
Agent category: | Peptide
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(USPIO-R832%20OR%20P03011))]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Endothelial cells are important cells in inflammatory responses (2, 3). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (4).

VCAM-1 is found in very low levels on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (5-9). VCAM-1 binds to the very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is also induced by oxidized low-density lipoproteins under atherogenic conditions (10). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression to vulnerable plaques, which may erode and rupture. CLIO nanoparticles targeted with anti-VCAM-1 antibody are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (11). A cyclic heptapeptide, cyclo(Cys-Asn-Asn-Ser-Lys-Ser-His-Thr-Cys) (R832), was identified with phage screening against VCAM-1 (12). Burtea et al. conjugated R832 to polyethylene glycol (PEG)–coated ultrasmall superparamagnetic iron oxide (USPIO) nanoparticles. USPIO-R832 (also known as P03011) was evaluated as a noninvasive MRI agent for VCAM-1 expression in vascular endothelial cells in atherosclerosis, vascular inflammation, and cerebral ischemia in mice (13-15).

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VCAM-1+AND+micad%5Bbook%5D), R832 (http://www.ncbi.nlm.nih.gov/books/?term=(R832+OR+P03011)+AND+micad%5Bbook%5D))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://omim.org/entry/192225))
- Clinical trials (VCAM-1 (http://www.clinicaltrials.gov/ct2/results?term=VCAM-1))
- Drug information in FDA (VCAM-1 (http://google2.fda.gov/search?q=VCAM-1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=11))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(USPIO-R832%20OR%20P03011)+synthesis)]

The synthesis of USPIO-R832 was described by Burtea et al. (13). A solution of 8-amino-3,6-dioxaoctanoyl-R832 with the Lys residue protected by reaction with trifluoroacetic acid to form amides (10 mg) and N-(3-dimethylaminopropyl)-N'-ethylcarbodiimide hydrochloride (EDCI) was added to USPIO nanoparticles and incubated for 20 h. The nanoparticles were isolated with ultrafiltration. A solution of the nanoparticles, EDCI, and aminoPEG750 was incubated for 17 h. The peptide was deprotected by hydrolysis (pH 10) for 6 h at room temperature. The product, USPIO-R832, was isolated with ultrafiltration. A nonspecific peptide (NSP) was also similarly conjugated to USPIO for use as control. The hydrodynamic diameters of USPIO-R832, USPIO-NSP, and USPIO-PEG (also known as P03007) were 26–27 nm. USPIO-R832, USPIO-NSP, and USPIO-PEG exhibited longitudinal (r_1_) relaxivity values of 1.9–2.2 mM−^1^s−^1^ at 7 T, and transverse (r_2_) relaxivity values of 85.9, 75.6, and 74.6 mM−^1^s−^1^ at 7 T, respectively. The number of peptides per USPIO-R832 nanoparticle was not reported. Michalska et al. (15) reported that there was one R832 peptide per P03011 nanoparticle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(USPIO-R832%20OR%20P03011)+in+vitro)]

Burtea et al. (12) measured the binding affinity of R832 to human VCAM-1 with a dissociation constant (K_d_) value of 103 nM. Saturation binding assays to human VCAM-1 were performed with various concentrations of USPIO-R832, which exhibited a K_d_ value of 37.2 nM (13). In vitro cellular accumulation of USPIO-R832 (37.2 nM, 4 mM Fe) and USPIO-PEG (4 mM Fe) assays were performed in human umbilical vein endothelial cells (HUVEC) before and after stimulation with TNFα_._ The cellular Fe level of USPIO-R832 was 170% higher in the stimulated cells than that in the non-stimulated cells and four- to six-fold higher than that of USPIO-PEG.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(USPIO-R832%20OR%20P03011)+rodentia)]

Burtea et al. (13) performed in vivo 4.7-T MRI in apolipoprotein E–deficient (apoE−^/^−) mice (n = 15) before and after injection of 0.1 mmol Fe/kg USPIO-R832, USPIO-NSP, or USPIO-PEG. There was −52% contrast in MRI signal intensity (ΔSNR) in the aortic wall at 32 min after injection of USPIO-R832. The aortic ΔSNR remained constant for up to 92 min of imaging and decreased to −18% at 24 h. The liver signals were −34%, −31%, and −63% at 33 min, 92 min, and 24 h, respectively. UPSIO-NSP exhibited aortic ΔSNR of −20% during the 92-min scans and decreased to −16% at 24 h. The liver signals were −11%, −20%, and −33% at 33 min, 92 min, and 24 h, respectively. USPIO-PEG produced aortic ΔSNR of −37% and −6% at 221 min and 24 h, respectively. The liver signals were 4%, 12%, and −30% at 33 min, 92 min, and 24 h, respectively. Immunohistological staining of the aorta sections of apoE−^/^− mice confirmed the presence of atherosclerotic lesions with extensive expression of VCAM-1. R832 colocalized with VCAM-1 and expression (r^2^ = 0.939). The blood elimination half-lives for USPIO-R832 and USPIO-PEG were 285 min and 443 min, respectively. Michalska et al. (15) reported a marked MRI signal loss (17.6 T) in the aortic root in apoE−^/^− mice injected with P03011. No blocking studies were performed.

Frechou et al. (14) performed in vivo 7-T MRI in mice with cerebral ischemia induced by occlusion of the left common carotid artery, followed by perfusion. P03011 (USPIO-R832) (n = 4) or P03007 (USPIO-PEG) (n = 4) (0.1 mmol Fe/kg) was injected intravenously at 5 h after the induction of cerebral ischemia. A lesion was located in both the cortex and striatum, with maximal VCAM-1 expression in the lesion at 24 h post-ischemia. In vivo MRI (T2*-weighted) was performed in the brain at 24 h after nanoparticle injection. The volume of hypointense pixels in the control normal mice was 272.6 ± 99.3 µl. Injection of P03007 had no effect on this volume, whereas injection of P03011 increased this volume by 1.6-fold (P < 0.05). Ex vivo T2*-weighted imaging exhibited a similar profile, with P03011 increasing the volume by four-fold (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(USPIO-R832%20OR%20P03011)+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(USPIO-R832%20OR%20P03011)+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(USPIO-R832%20OR%20P03011)+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
3 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
4 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
5 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
6 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
7 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
8 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
9 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
10 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
11 Tsourkas A., Shinde-Patil V.R., Kelly K.A., Patel P., Wolley A., Allport J.R., Weissleder R. (2005). In vivo imaging of activated endothelium using an anti-VCAM-1 magnetooptical probe. Bioconjug Chem.
12 Burtea C., Laurent S., Port M., Lancelot E., Ballet S., Rousseaux O., Toubeau G., Vander Elst L., Corot C., Muller R.N. (2009). Magnetic resonance molecular imaging of vascular cell adhesion molecule-1 expression in inflammatory lesions using a peptide-vectorized paramagnetic imaging probe. J Med Chem.
13 Burtea C., Ballet S., Laurent S., Rousseaux O., Dencausse A., Gonzalez W., Port M., Corot C., Vander Elst L., Muller R.N. (2012). Development of a magnetic resonance imaging protocol for the characterization of atherosclerotic plaque by using vascular cell adhesion molecule-1 and apoptosis-targeted ultrasmall superparamagnetic iron oxide derivatives. Arterioscler Thromb Vasc Biol.
14 Frechou M., Beray-Berthat V., Raynaud J.S., Meriaux S., Gombert F., Lancelot E., Plotkine M., Marchand-Leroux C., Ballet S., Robert P., Louin G., Margaill I. (2013). Detection of vascular cell adhesion molecule-1 expression with USPIO-enhanced molecular MRI in a mouse model of cerebral ischemia. Contrast Media Mol Imaging.
15 Michalska M., Machtoub L., Manthey H.D., Bauer E., Herold V., Krohne G., Lykowsky G., Hildenbrand M., Kampf T., Jakob P., Zernecke A., Bauer W.R. (2012). Visualization of vascular inflammation in the atherosclerotic mouse by ultrasmall superparamagnetic iron oxide vascular cell adhesion molecule-1-specific nanoparticles. Arterioscler Thromb Vasc Biol.